# 3-[3,5-Dimethyl-4-(4-[^11^C]methylpiperazinecarbonyl)-1H-pyrrol-2-ylmethylene]-2-oxo-2,3-dihydro-1H-indole-5-sulfonic acid (3-chlorophenyl)methylamide

Chemical name: | 3-[3,5-Dimethyl-4-(4-[^11^C]methylpiperazinecarbonyl)-1H-pyrrol-2-ylmethylene]-2-oxo-2,3-dihydro-1H-indole-5-sulfonic acid (3-chlorophenyl)methylamide
Abbreviated name: | [^11^C]SU11274
Synonym:
Agent category: | Compound
Target: | MET, also known as the tyrosine kinase receptor for hepatocyte growth factor
Target category: | Receptor
Method of detection: | Positron emission tomography (PET)
Source of signal: | ^11^C
Activation: | No
Studies: | - In vitro; - Rodents | Click on the above structure for additional information in PubChem (http://pubchem.ncbi.nlm.nih.gov/).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=SU11274)]

MET is a proto-oncogene that encodes a protein Met, also known as c-Met or hepatocyte growth factor receptor (HGFR) (1). MET is a membrane receptor with tyrosine kinase activity that is essential for embryonic development and wound healing. MET is normally expressed by stem cells, progenitor cells, and cells of epithelial origin, whereas expression of hepatocyte growth factor (HGF), which is the only known ligand of MET, is restricted to cells of mesenchymal origin. Upon HGF stimulation, MET induces several biological responses that lead to invasive growth (2). Abnormal MET activation in cancer correlates with poor prognosis because deregulated MET triggers tumor growth, induces angiogenesis, and activates metastasis (3). MET is deregulated in many types of human malignancies, including kidney, liver, stomach, breast, and brain cancers (2, 4, 5). Inhibition of MET function has been shown to inhibit pathological angiogenesis as well as tumor growth and metastasis (6). 3-[3,5-Dimethyl-4-(4-methylpiperazinecarbonyl)-1H-pyrrol-2-ylmethylene]-2-oxo-2,3-dihydro-1H-indole-5-sulfonic acid (3-chlorophenyl)methylamide (SU11274) is directed against the MET kinase activity that leads to apoptosis and inhibition of cell growth (7). Wu et al. (8) reported the use of 3-[3,5-dimethyl-4-(4-[^11^C]methylpiperazinecarbonyl)-1H-pyrrol-2-ylmethylene]-2-oxo-2,3-dihydro-1H-indole-5-sulfonic acid (3-chlorophenyl)methylamide ([^11^C]SU11274) for positron emission tomography (PET) imaging of MET expression in human lung xenografts in mice.

### Related Resource Links:

- Chapters in MICAD (c-Met (http://www.ncbi.nlm.nih.gov/sites/entrez?db=Books&cmd=Search&term=c-Met+AND+micad%5bbook%5d&doptcmdl=TOCView&log%24=booksrch&bname=micad))
- Gene information in NCBI (c-Met (http://www.ncbi.nlm.nih.gov/gene/4233)).
- Articles in Online Mendelian Inheritance in Man (OMIM) (c-Met (http://www.ncbi.nlm.nih.gov/omim/?term=c-Met))
- Clinical trials (c-Met (http://www.clinicaltrials.gov/ct2/results?term=c-Met))
- Drug information in FDA (c-Met (http://google2.fda.gov/search?q=c-Met&client=FDAgov&site=FDAgov&lr=&proxystylesheet=FDAgov&output=xml_no_dtd&getfields=*&x=10&y=12))

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=SU11274+synthesis)]

[^11^C]SU11274 was synthesized by alkylation of the precursor 3-[3,5-dimethyl-4-(piperazine-1-carbonyl)-1H-pyrrol-2-ylmethylene]-2-oxo-2,3-dihydro-1H-indole-5-sulfonic acid (3-chlorophenyl)methylamide hydrochloride with [^11^C]methyl iodide (8). Subsequent high-performance liquid chromatography separation resulted in a 5–10% (decay-corrected) radiochemical yield based on [^11^C]methyl iodide, with a total synthesis time of 30–40 min from the end of bombardment and a radiochemical purity >98%. The specific activity was 11.1–18.5 GBq/mmol (0.3–0.5 Ci/mmol) at the end of synthesis.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=SU11274+in+vitro)]

In vitro kinase inhibition assays were performed with various recombinant receptor kinases (7). SU11274 had a 50% inhibition concentration (IC_50_) value of 20 nM for MET. The IC_50_ values of SU11274 for various tyrosine kinases (Flk, EGFR, PDGFR, Tie2, c-src, edk2, and FGFR-1) were determined to be >50–fold greater than that for MET.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=SU11274+rodentia)]

Wu et al. (8) performed PET studies of 18.5 MBq (0.5 mCi) [^11^C]SU11274 in nude mice bearing human lung cancer xenografts of NCI-H1975 (high MET expression) or NCI-H520 (low MET expression) tumor cell lines. NCI-H1975 tumor standard uptake values (SUVs) were 0.32 at 10 min, 0.42 at 65 min, and 0.46 at 80 min. These SUVs were 35%, 110%, and 160% higher (P < 0.01) than those for NCI-H520 tumors at these time points, respectively. NCI-H1975 tumors but not NCI-H520 tumors were readily visualized during the 90 min of imaging. Immunohistochemistry performed on NCI-H1975 and NCI-H520 xenografts showed that the expression of MET was present in the NCI-H1975 tumor sections but absent in the NCI-H520 tumor sections. No blocking experiments were performed, but the use of a high-expression tumor and a low-expression tumor supports the specificity of localization.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=SU11274+and+(dog+or+sheep+or+pig+or+rabbit))]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=SU11274+and+(primate+not+human))]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=SU11274+human)]

No publication is currently available.

## NIH Support

5K08 CA102545-04

## References

1 Boccaccio C., Comoglio P.M. (2006). Invasive growth: a MET-driven genetic programme for cancer and stem cells. Nat Rev Cancer.
2 Di Renzo M.F., Olivero M., Giacomini A., Porte H., Chastre E., Mirossay L., Nordlinger B., Bretti S., Bottardi S., Giordano S., et al. (1995). Overexpression and amplification of the met/HGF receptor gene during the progression of colorectal cancer. Clin Cancer Res.
3 Lengyel E., Prechtel D., Resau J.H., Gauger K., Welk A., Lindemann K., Salanti G., Richter T., Knudsen B., Vande Woude G.F., Harbeck N. (2005). C-Met overexpression in node-positive breast cancer identifies patients with poor clinical outcome independent of Her2/neu. Int J Cancer.
4 Smith H.S., Stern R., Liu E., Benz C. (1991). Early and late events in the development of human breast cancer. Basic Life Sci.
5 Di Renzo M.F., Olivero M., Serini G., Orlandi F., Pilotti S., Belfiore A., Costantino A., Vigneri R., Angeli A., Pierotti M.A., et al. (1995). Overexpression of the c-MET/HGF receptor in human thyroid carcinomas derived from the follicular epithelium. J Endocrinol Invest.
6 Petrelli A., Circosta P., Granziero L., Mazzone M., Pisacane A., Fenoglio S., Comoglio P.M., Giordano S. (2006). Ab-induced ectodomain shedding mediates hepatocyte growth factor receptor down-regulation and hampers biological activity. Proc Natl Acad Sci U S A.
7 Sattler M., Pride Y.B., Ma P., Gramlich J.L., Chu S.C., Quinnan L.A., Shirazian S., Liang C., Podar K., Christensen J.G., Salgia R. (2003). A novel small molecule met inhibitor induces apoptosis in cells transformed by the oncogenic TPR-MET tyrosine kinase. Cancer Res.
8 Wu C., Tang Z., Fan W., Zhu W., Wang C., Somoza E., Owino N., Li R., Ma P.C., Wang Y. (2010). In vivo positron emission tomography (PET) imaging of mesenchymal-epithelial transition (MET) receptor. J Med Chem.